# (S)-1-(4-(2-[^18^F]Fluoroethoxy)benzyl)-5-[1-(2-methoxymethyl-pyrrolidinyl)sulfonyl]-1H-indole-2,3-dione

Chemical name: | (S)-1-(4-(2-[^18^F]Fluoroethoxy)benzyl)-5-[1-(2-methoxymethyl-pyrrolidinyl)sulfonyl]-1H-indole-2,3-dione
Abbreviated name: | [^18^F]CbR2
Synonym:
Agent category: | Compound
Target: | Caspase-3
Target category: | Enzyme
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20isatin)]

Apoptosis (programmed cell death) plays an important role in the pathophysiology of many diseases, such as cancer, neurodegenerative disorders, vascular disorders, and chronic hepatitis, as well as in the biology of normal cells, such as epithelial cells and immune cells (1). Apoptosis is gene-regulated (2) and is the result of proteolysis of intracellular components by activation of a series of proteolytic enzymes called caspases and changes of plasma membrane structure by translocase, floppase, and scramblase (3-5). As a result, there is rapid redistribution of phosphatidylserine (PS) from the inner membrane leaflet to the outer membrane leaflet, exposing the anionic head group of PS. On the other hand, PS is also accessible for annexin V binding in necrosis because of disruption of the plasma membrane.

Annexin V is a 36-kDa endogenous human protein produced in particular by epithelial cells from many tissues, such as the placenta, umbilical vessels, liver, spleen, kidney, heart, uterus, and skeletal muscle, as well as by erythrocytes, leukocytes, endothelial cells, and platelets (6). Annexin V binds to PS with high affinity (K_d_ = 7 nM) (3, 7, 8). Apoptosis can be induced by chemicals, radiation, cytokines, hormones, and various pathological conditions (5); therefore, the ability to monitor apoptosis in association with disease progression or regression should provide important information for clinical applications. Annexin V has been radiolabeled with ^18^F, ^123^I, ^125^I, and ^99m^Tc for imaging (9-12). However, annexin V is not able to distinguish between apoptosis and necrosis. Caspase ligand may be an attractive alternative for imaging cells undergoing apoptosis because caspases are key enzymes that mediate apoptosis (13). Kopka et al. (14) reported that 5-pyrrolidinylsulfonyl isatins exhibited selective inhibition of caspase-3 and caspase-7 (executioner caspases) over caspase-1, -6, and -8 (initiator caspases). (S)-1-(4-(2-[^18^F]Fluoroethoxy)benzyl)-5-[1-(2-methoxymethyl-pyrrolidinyl)sulfonyl]-1H-indole-2,3-dione ([^18^F]CbR2), one of the N-1–substituted 5-pyrrolidinylsulfonyl isatin analogs, has been synthesized for imaging caspase-3 activation in apoptosis (15).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20isatin%20and%20synthesis)]

Faust et al. (15) report the synthesis of [^18^F]CbR2 by nucleophilic displacement of the tosylate group of the tosylate precursor with [^18^F]KF (Kryptofix 2.2.2./K_2_CO_3_) at 85°C for 5 min. Subsequent high-performance liquid chromatography separation gave radiochemical yields of ~32% (decay-corrected) and radiochemical purities >90% with a total synthesis time of 82 min. The specific activity was 48 GBq/μmol (1.3 Ci/μmol) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20isatin%20and%20in%20vitro)]

In vitro caspase enzyme assays using CbR2 showed inhibition concentration (IC_50_) values of 36.4 ± 5.5 nM for caspase-3, 93.3 ± 1.0 nM for caspase-7, and >25,000 nM for caspase-6, -1, and -8 (14).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20isatin%20and%20rodentia)]

Faust et al. (15) performed a preliminary biodistribution study in nude mice (n = 2/group) at 10 and 32 min after injection of 7 MBq (0.19 mCi) [^18^F]CbR2. The highest accumulation of radioactivity was observed at 10 min after injection in the gall bladder, followed by the duodenum, liver, and kidney. Radioactivity in the blood and most peripheral organs was cleared by 32 min, with the main fraction of radioactivity remaining in the urinary bladder. The microPET imaging at 165–180 min confirmed that the radioactivity remained in the liver, bowels, and urinary bladder as observed in the biodistribution study. The authors suggested that further preclinical in vivo studies are needed to confirm the usefulness of [^18^F]CbR2 as a caspase-3 probe in imaging apoptosis in humans.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20isatin%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20isatin%20and%20%28primate%20not%20human%29)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20isatin%20and%20human)]

No publications are currently available.

## NIH Support

HL13851, EB 001729, CA121952

## References

1 Thompson C.B. (1995). Apoptosis in the pathogenesis and treatment of disease. Science.
2 Steller H. (1995). Mechanisms and genes of cellular suicide. Science.
3 Thiagarajan P., Tait J.F. (1990). Binding of annexin V/placental anticoagulant protein I to platelets. Evidence for phosphatidylserine exposure in the procoagulant response of activated platelets. J Biol Chem.
4 Song Z., Steller H. (1999). Death by design: mechanism and control of apoptosis. Trends Cell Biol.
5 Blankenberg F.G., Tait J., Ohtsuki K., Strauss H.W. (2000). Apoptosis: the importance of nuclear medicine. Nucl Med Commun.
6 Blankenberg F.G., Strauss H.W. (2001). Will imaging of apoptosis play a role in clinical care? A tale of mice and men. Apoptosis.
7 van Heerde W.L., de Groot P.G., Reutelingsperger C.P. (1995). The complexity of the phospholipid binding protein Annexin V. Thromb Haemost.
8 Tait J.F., Cerqueira M.D., Dewhurst T.A., Fujikawa K., Ritchie J.L., Stratton J.R. (1994). Evaluation of annexin V as a platelet-directed thrombus targeting agent. Thromb Res.
9 Blankenberg F.G. (2004). Recent advances in the imaging of programmed cell death. Curr Pharm Des.
10 Lahorte C., Slegers G., Philippe J., Van de Wiele C., Dierckx R.A. (2001). Synthesis and in vitro evaluation of 123I-labelled human recombinant annexin V. Biomol Eng.
11 Toretsky J., Levenson A., Weinberg I.N., Tait J.F., Uren A., Mease R.C. (2004). Preparation of F-18 labeled annexin V: a potential PET radiopharmaceutical for imaging cell death. Nucl Med Biol.
12 Zijlstra S., Gunawan J., Burchert W. (2003). Synthesis and evaluation of a 18F-labelled recombinant annexin-V derivative, for identification and quantification of apoptotic cells with PET. Appl Radiat Isot.
13 Neuss M., Crow M.T., Chesley A., Lakatta E.G. (2001). Apoptosis in cardiac disease--what is it--how does it occur. Cardiovasc Drugs Ther.
14 Kopka K., Faust A., Keul P., Wagner S., Breyholz H.J., Holtke C., Schober O., Schafers M., Levkau B. (2006). 5-pyrrolidinylsulfonyl isatins as a potential tool for the molecular imaging of caspases in apoptosis. J Med Chem.
15 Faust A., Wagner S., Law M.P., Hermann S., Schnockel U., Keul P., Schober O., Schafers M., Levkau B., Kopka K. (2007). The nonpeptidyl caspase binding radioligand (S)-1-(4-(2-[(18)F]Fluoroethoxy)-benzyl)-5-[1-(2-methoxymethylpyrrolidinyl) sulfonyl]isatin ([18F]CbR) as potential positron emission tomography-compatible apoptosis imaging agent. Q J Nucl Med Mol Imaging.